# ^99m^Tc-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_

Chemical name: | ^99m^Tc-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_ | [image]
Abbreviated name: | ^99m^Tc-(Arg^11^)CCMSH | [image]
Synonym: | ^99m^Tc-α-MSH, ^99m^Tc-Labeled α-melanocyte−stimulating hormone peptides | [image]
Backbone: | Peptide | [image]
Target: | Melanocortin-1 (MC-1) receptor | [image]
Mechanism: | Peptide-receptor binding | [image]
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging | [image]
Source of signal: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | ^99m^Tc-(Arg^11^)CCMSH structure. Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=27477129), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=27477128) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=4157) for more information about the melanocortin-1 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-%20and%20111In-labeled%20alpha-melanocyte-stimulating%20hormone%20peptides%29%20OR%20%28radiolabeled-alpha-MSH%29)]

^99m^Tc-[Cys^3,4,10^,D-Phe^7^,Arg^11^]αMSH_3-13_ (^99m^Tc-(Arg^11^)CCMSH) is a radioligand developed as a single-photon emission computed tomography (SPECT) imaging probe for primary and metastatic melanoma (1). ^99m^Tc-(Arg^11^)CCMSH is an α-melanocyte−stimulating hormone (MSH) peptide labeled with ^99m^Tc, a gamma emitter with a physical t_½_ of 6 h.

Malignant melanoma is the sixth most common cancer in the United States (1). Early diagnosis and prompt surgical removal comprise the best approach for a possible cure (2). The melanocortin (MC) system is the best characterized neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production and many other physiological processes (3). Most cutaneous cell types express MC receptors, proopiomelanocortin (POMC), prohormone convertases, and also release MCs. Five MC receptors (MC-1 to MC-5) have been cloned and characterized as receptors that belong to the G-protein−coupled receptors superfamily. MSHs (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_) is a 13−amino acid peptide and is the most potent naturally occurring melanotropic peptide (4). The biological effects of α-MSH are mediated via MC receptors.

Although positron emission tomography (PET) imaging with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) is effective in the detection of melanoma, it is not melanoma-specific and some melanoma cells do not take up [^18^F]FDG (5, 6). Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC-1 receptors which are overexpressed on human and mouse melanoma cells (5, 7-10). Some studies have successfully used 1,4,7,10-tetraazacyclodecane-N,N',N'',N'''-tetraacetic acid (DOTA) coupled to the α-MSH peptide analogs for radiolabeling. These α-MSH derivatives (DOTA-α-MSH) can be labeled with a variety of radionuclides (5). To improve the in vivo pharmacokinetics of these radiolabeled peptides, a number of different α-MSH analogs have been designed (11, 12). Froidevaux et al. (11) showed that the kidney uptake of a short linear DOTA−α-MSH analog (DOTA-NAPamide) could be considerably reduced by neutralizing the charge of the Lys^11^ residue. Giblin et al. (13) used metal cyclization to design a new class of α-MSH peptide analogs that are resistant to chemical and proteolytic degradation in vivo (10). ^99m^Tc-CCMSH analogs, cyclized through site-specific coordination of ^99m^TcO, showed excellent tumor uptake and retention properties in B16/F1 murine melanoma-bearing C57 mice (13, 14). Miao et al. (12) replaced the Lys^11^ with Arg^11^ in the CCMSH analog to form (Arg^11^)CCMSH in an effort to reduce nonspecific kidney uptake and minimize the kidney radiation dose.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-%20and%20111In-labeled%20alpha-melanocyte-stimulating%20hormone%20peptides%29%20OR%20%28radiolabeled-alpha-MSH%29%20AND%20synthesis)]

Miao et al. (12) reported the synthesis of the (Arg^11^)CCMSH by using the standard fluorenylmethoxycarbonyl (Fmoc)/HBTU chemistry on amide resin. A solid-phase peptide synthesizer was used. The peptide was acetylated with glacial acetic acid at the N-terminus. The peptide was deprotected and cleaved from the resin by a mixture of trifluoroacetic acid, thioanisol, ethanedithiol, and water at room temperature for 3 h. The peptide was then purified by high-performance liquid chromatography (HPLC), and the identity was confirmed by electrospray ionization mass spectrometry. The ^99m^Tc radiolabeling was prepared via a glucoheptonate transchelation reaction (14).In this procedure, stannous chloride (SnCl_2_) was used as a reducing agent and glucoheptonate was used as a transfer ligand. Briefly, 10 μg of the peptide was added to the mixture of SnCl_2_, ^99m^Tc-pertechnetate, and glucoheptonate. The mixture was incubated at 75ºC for 30 min. The final ^99m^Tc-(Arg^11^)CCMSH product was purified by HPLC. The specific activity was 1.2135 x 10^10^ MBq/g (3.280 x 10^8^ mCi/g). Based on a molecular weight of 1,467, the specific activity can be estimated to be 1.79 x 10^7^ MBq/μmol (48.4 x 10^4^ mCi/μmol).The radiochemical stability was evaluated in phosphate- buffered saline (pH 7.4). Over a 24-h period of incubation at 25ºC in phosphate-buffered saline, only radiolabeled peptide was detected by HPLC analysis with no detectable free radioactivity (14).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-%20and%20111In-labeled%20alpha-melanocyte-stimulating%20hormone%20peptides%29%20OR%20%28radiolabeled-alpha-MSH%29%29%20AND%20in%20vitro)]

Giblin et al. (13) performed in vitro quantitative receptor-binding assays of unlabeled CCMSH on B16/F1 murine melanoma cells. The inhibition constant (IC_50_) was determined to be 7.6 x 10−^9^ M. Miao et al. (12) determined the IC_50_ of unlabeled (Arg^11^)CCMSH to be 1.7 X 10−^9^ M, and the molecular weight was measured to be 1,476.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-%20and%20111In-labeled%20alpha-melanocyte-stimulating%20hormone%20peptides%29%20OR%20%28radiolabeled-alpha-MSH%29%29%20AND%20rodentia)]

Biodistribution and SPECT imaging studies with ^99m^Tc-(Arg^11^)CCMSH were conducted in C57 mice bearing B16/F1 (flank melanoma tumors) and B16/F10 (pulmonary metastatic melanoma tumors) melanomas (1). Each mouse received 27.75 MBq (0.75 mCi) of ^99m^Tc-(Arg^11^)CCMSH by i.v. administration. The radioactivity levels in the flank tumors (n = 4) were 14.03 ± 2.58 (1 h), 11.16 ± 1.77 (4 h), and 3.33 ± 0.50 (24 h) % injected dose per g (% ID/g). The tumor/muscle ratios were 61 (1 h), 372 (4 h), and 333 (24 h). The critical organ appeared to be the kidneys (% ID/g) with 11.66 ± 1.44 (1 h), 5.53 ± 1.17 (4 h), and 0.60 ± 0.08 (24 h). The other major organ radioactivity levels (% ID/g) at 1 h were 7.32 ± 1.28 (intestines), 3.00 ± 0.45 (stomach), 1.59 ± 0.19 (liver), 1.52 ± 0.39 (lung), 1.97 ± 0.37 (skin), 0.63 ± 0.17 (heart), 0.04 ± 0.02 (brain), 0.23 ± 0.06 (muscle), and 0.87 ± 0.12 (blood). With coinjection of 10 μg of a high- affinity unlabeled αMSH analog, NDP ([NIe^4^,D-Phe^7^] αMSH), the tumor radioactivity was reduced by 90% (1.44 ± 0.23% ID/g) at 1 h.

In the pulmonary metastatic tumor model, the radioactivity levels (% ID/g) of ^99m^Tc-(Arg^11^)CCMSH in the lung metastases (n = 4) were 2.77 ± 0.98 (2 h) and 2.30 ± 1.78 (4 h) (1). The radioactivity levels in the normal lung were 0.52 ± 0.22 (2 h) and 0.65 ± 0.13 (4 h). The lung metastases/normal lung ratios were 5.33 and 3.54 at 2 h and 4 h, respectively. The lung metastases/muscle ratios were 11.54 and 5.00 at 2 h and 4 h, respectively. In the imaging studies, the flank melanoma tumors were visualized clearly at 2 h. The pulmonary metastatic melanoma lesions were also clearly imaged at 2 h, and distinct metastatic focal deposits were visible.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-%20and%20111In-labeled%20alpha-melanocyte-stimulating%20hormone%20peptides%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-%20and%20111In-labeled%20alpha-melanocyte-stimulating%20hormone%20peptides%29%20OR%20%28radiolabeled-alpha-MSH%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-%20and%20111In-labeled%20alpha-melanocyte-stimulating%20hormone%20peptides%29%20OR%20%28radiolabeled-alpha-MSH%29%29%20AND%20human)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

NCI P50-CA-103130

## References

1 Miao Y., Benwell K., Quinn T.P. (2007). 99mTc- and 111In-labeled alpha-melanocyte-stimulating hormone peptides as imaging probes for primary and pulmonary metastatic melanoma detection. J Nucl Med.
2 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
3 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
4 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
5 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
6 Dimitrakopoulou-Strauss A., Strauss L.G., Burger C. (2001). Quantitative PET studies in pretreated melanoma patients: a comparison of 6-[18F]fluoro-L-dopa with 18F-FDG and (15)O-water using compartment and noncompartment analysis. J Nucl Med.
7 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
8 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
9 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
10 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
11 Froidevaux S., Calame-Christe M., Tanner H., Eberle A.N. (2005). Melanoma targeting with DOTA-alpha-melanocyte-stimulating hormone analogs: structural parameters affecting tumor uptake and kidney uptake. J Nucl Med.
12 Miao Y., Owen N.K., Whitener D., Gallazzi F., Hoffman T.J., Quinn T.P. (2002). In vivo evaluation of 188Re-labeled alpha-melanocyte stimulating hormone peptide analogs for melanoma therapy. Int J Cancer.
13 Giblin M.F., Wang N., Hoffman T.J., Jurisson S.S., Quinn T.P. (1998). Design and characterization of alpha-melanotropin peptide analogs cyclized through rhenium and technetium metal coordination. Proc Natl Acad Sci U S A.
14 Chen J., Cheng Z., Hoffman T.J., Jurisson S.S., Quinn T.P. (2000). Melanoma-targeting properties of (99m)technetium-labeled cyclic alpha-melanocyte-stimulating hormone peptide analogues. Cancer Res.